# ^18^F-Labeled N-(4-fluorobenzylidene)oxime-dimeric (Z_HER2:477_)_2_

Chemical name: | ^18^F-N-(4-fluorobenzylidene)oxime-dimeric (Z_HER2:477_)_2_ | [image]
Abbreviated name: | ^18^F-FBO-(Z_HER2:477_)_2_ | [image]
Synonym: | | [image]
Agent Category: | Affibody, antibody | [image]
Target: | HER2 | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of the agents by Cheng et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=affibody%20and%20HER2%20and%20molecular%20imaging)]

The ^18^F-labeled N-(4-fluorobenzylidene)oxime (FBO)-dimeric (Z_HER2:477_)_2_ conjugate, abbreviated as ^18^F-FBO-(Z_HER2:477_)_2_, is an affibody derivative synthesized by Cheng et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that derive from the B-domain of staphylococcal surface protein A (2, 3). In the past several years, affibodies have drawn significant attention for developing imaging and therapeutic agents because of their unique features (3, 4). First, affibodies are small, with only 58 amino acid residues (~7 kDa) (3, 5). The small size allows affibodies to be generated with solid-phase peptide synthesis and to be cleared quickly from kidneys. Second, affibodies have a high binding affinity and specificity to their targets. Their binding affinity can be further improved by generating multimeric constructs through the solvent-exposed termini of affibody Z-domain. The anti-HER2 monomeric affibody Z_HER2:4_ is an example that has a binding affinity of ~50 nM, but its dimeric form, (Z_HER2:4_)_2_, exhibits an improved binding affinity of up to ~3 nM in vitro (6). Third, affibodies lack cysteine residues and disulfide bridges in structure, and they fold rapidly. These features make it possible to chemically synthesize fully functional molecules and to introduce unique cysteine residues or chemical groups into affibodies for site-specific labeling. Several anti-HER2 affibody derivatives have been synthesized in this way. The imaging agent HPEM-His_6_-(Z_HER2:4_)_2_-Cys was generated by radiobrominating the dimeric (Z_HER2:4_)_2_ through the cysteine residues that were introduced to the C-terminus of (Z_HER2:4_)_2_ (7). Several affibody derivatives (e.g., ^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), and ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/)) were synthesized by coupling a chelating agent with a specifically protected site group of the Z_HER2:342_ peptide chain (3). Furthermore, affibody proteins can be selected and optimized with a strategy of sequence mutation and affinity maturation, and an example selected with this strategy is the anti-HER2 affibody Z_HER2:342_, which has an increased affinity of 50 nM (Z_HER2:4_, the first generation) to 22 pM (8).

The investigators at Stanford University first tested the feasibility of the monomeric and dimeric forms of anti-HER2 affibody Z_HER2:477_ for molecular imaging. Both forms of the Z_HER2:477_ molecule were radiofluorinated with an ^18^F-labeled prosthetic group of 4-^18^F-fluorobenzaldehyde (^18^F-FBO-Z_HER2:477_ and ^18^F-FBO-(Z_HER2:477_)_2_, respectively) (1). The investigators have also coupled ^64^Cu to the affibody through DOTA, leading to the development of imaging agents ^64^Cu-DOTA- Z_HER2:477_ and ^64^Cu-DOTA-(Z_HER2:477_)_2_ (9). Interestingly, these studies showed that smaller affibody constructs performed better in vivo in terms of tumor uptake and clearance in spite of the lower affinity in vitro. The investigators then generated a class of small proteins consisting of two α-helix bundles of the 3-helix affibody by deleting the helix 3 because the binding domain localizes in the α-helices 1 and 2 bundles (5). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles, with a disulfide bridge being formed between the two inserted homocysteines (10-12). MUT-DS showed a binding affinity to HER2 in the low-nM range. The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for both imaging and therapy of HER2-expressing tumors (refer to MUT-DS derived agents in MICAD).

This series of chapters summarizes the data obtained with the Z_HER2:477_ derivatives, and this chapter presents the data obtained with ^18^F-FBO-(Z_HER2:477_)_2_ (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-Benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-Benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/)

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/18413392)]

The dimeric affibody (Z_HER2:477_)_2_ with distal C-terminal cysteine residues (purity, >95%) is commercially available. The agent ^18^F-FBO-(Z_HER2:477_)_2_ was synthesized in three steps (1). The bifunctional linker 2-(aminooxy)-N-(2-(2,5-dioxo-2,5-dihydro-^1^H-pyrrol-1-yl)ethyl)acetamide hydrochloride was first prepared by reacting N-(2-aminoethyl)malemide with 2-(tert-butoxycarbonylaminooxy)acetic acid under carbodiimide-mediated coupling conditions. The linker consisted of two orthogonal groups, a thiol-reactive maleimide group for conjugation to the cysteine residue and an ^18/19^F-aldehyde–reactive aminooxy group. The yield was 80%. The linker was then selectively conjugated to the affibody molecule to generate aminooxy-functionalized (Z_HER2:477_)_2_ ((Z_HER2:477_)_2_-ONH_2_; yield = 79%; molecular weight (MW) = 14,431.26 Da). As the last step, (Z_HER2:477_)_2_-ONH_2_ was conjugated with 4-fluorobenzaldehyde (4-FBA), which resulted in the nonradioactive FBO-(Z_HER2:477_)_2_. The recovery yield was 70%–90%, and the measured MW was 14,538.59 Da for the nonradioactive FBO-(Z_HER2:477_)_2_. Similarly, conjugation of the (Z_HER2:477_)_2_-ONH_2_ with 4-^18^F-FBA led to the generation of radioactive ^18^F-FBO-(Z_HER2:477_)_2_. For radiolabeling, the coupling yield was 30%–40%, and the overall radiochemical yield ranged from 13% to 18% (end of synthesis, corrected for decay). The specific activity and purity of ^18^F-FBO-(Z_HER2:477_)_2_ were 10.4–20.8 MBq/nmol (20–40 μCi/μg) and >95%, respectively, at end of synthesis. The total synthesis time was ~100 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/18413392)]

Binding affinity with the extracellular domain of HER2 antigen was measured in vitro with surface plasmon resonance detection (1). The measurements showed that the binding affinities of (Z_HER2:477_)_2_-ONH_2_ and FBO-(Z_HER2:477_)_2_ were 180 and 200 pM, respectively (400 and 430 pM for the monomeric forms Z_HER2:477_-ONH_2_ and FBO-Z_HER2:477_, respectively). The association constants were in the range of 10^5^–10^6^ (association time, >2 min), and the dissociation constants were in the range of 10^-4^–10^-5^ (disassociation time, >15 min), indicating that the on rate was very fast and the off rate was very slow.

The HER2-targeting ability for cultured cells was evaluated with SKOV3 human ovarian cancer cells (0.2 × 10^6^ cells/well) after incubation for 2 h with 1.11−6.29 kBq (0.03–0.17 μCi) ^18^F-FBO-(Z_HER2:477_)_2_. ^18^F-FBO-(Z_HER2:477_)_2_ quickly accumulated in the SKOV3 cells and reached the value of 0.01447 cell counts per minute [cpm]/medium cpm/μg of protein/μL at 0.5 h, which was three-fold higher than that of the monomeric form. The uptake was maintained at almost the same level until 2 h. In the presence of a large excess of nonradioactive (Z_HER2:477_)_2_ (final concentration, 1.43 μM), the cell uptake of ^18^F-FBO-(Z_HER2:477_)_2_ was inhibited significantly at all incubation time points (P < 0.05), showing a value of only 0.00623 at 0.5 h, which suggests that the agent is specific to HER2 (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/18413392)]

Biodistribution studies were performed in nude mice bearing SKOV3 tumors (n = 3/time point) (1). Mice were injected via the tail vein with 0.74–1.665 MBq (20–45 μCi) ^18^F-FBO-(Z_HER2:477_)_2_ and then euthanized at different time points after injection. The radioactivity in ex vivo tissues was expressed as a percentage of the injected radioactive dose per gram of tissue (% ID/g). The accumulation of ^18^F-FBO-(Z_HER2:477_)_2_ in SKOV3 tumors was 2.03 ± 0.31% and 1.08 ± 0.15% ID/g at 0.5 h and 3 h after injection, respectively.

Compared to the monomeric form (refer to the chapter of ^18^F-FBO-Z_HER2:477_ in MICAD), ^18^F-FBO-(Z_HER2:477_)_2_ showed significantly lower tumor uptake and tumor/normal tissue (blood, muscle, liver, and lung) ratios at all time points (P < 0.5) in spite of the much higher affinity. Both monomeric and dimeric forms displayed relatively rapid blood clearance, with blood uptake values of 3.81 ± 0.50% and 1.97 ± 0.24% ID/g at 0.5 h (P < 0.05), respectively, and 1.50 ± 0.35% and 1.56 ± 0.29% ID/g at 1 h after injection, respectively. In the kidneys, both forms displayed very high levels of uptake, especially at the early time points (>20% ID/g at 0.5 h after injection), and the monomeric form had a comparatively higher renal uptake than the dimeric form. On the contrary, the dimeric form showed significantly higher levels of uptake in the liver and muscle at 0.5 h after injection than the monomeric form, but both forms displayed similar levels of uptake at later time points.

PET imaging was performed in mice bearing SKOV3 tumors at 0.5, 1, 2, and 4 h after tail vein injection of ^18^F-FBO-Z_HER2:477_ (0.444–0.814 MBq (12–22 μCi)) or ^18^F-FBO-(Z_HER2:477_)_2_ (1.85–2.035 MBq (50–55 μCi)) (1). The tumor was visible with both forms, especially at later time points, but a better tumor/background contrast was observed with the monomeric form. ^18^F-FBO-Z_HER2:477_ had approximately two-fold higher tumor uptake than ^18^F-FBO-(Z_HER2:477_)_2_. High levels of activity accumulation were observed in the kidneys and the intestinal tract for both forms.

In conclusion, studies by Cheng et al. showed that ^18^F-FBO-Z_HER2:477_ rapidly localized in SKOV3 tumors and exhibited good tumor uptake, retention, tumor/muscle ratio, and high specificity to HER2 (1). In contrast, ^18^F-FBO-(Z_HER2:477_)_2_ showed poor in vivo performance, although it had a higher affinity with HER2 and a higher cell uptake in vitro. ^18^F-FBO-Z_HER2:477_ is more promising than its dimeric form as an agent for HER2 imaging (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Tolmachev V., Orlova A., Nilsson F.Y., Feldwisch J., Wennborg A., Abrahmsen L. (2007). Affibody molecules: potential for in vivo imaging of molecular targets for cancer therapy. Expert Opin Biol Ther.
5 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
6 Steffen A.C., Wikman M., Tolmachev V., Adams G.P., Nilsson F.Y., Stahl S., Carlsson J. (2005). In vitro characterization of a bivalent anti-HER-2 affibody with potential for radionuclide-based diagnostics. Cancer Biother Radiopharm.
7 Mume E., Orlova A., Larsson B., Nilsson A.S., Nilsson F.Y., Sjoberg S., Tolmachev V. (2005). Evaluation of ((4-hydroxyphenyl)ethyl)maleimide for site-specific radiobromination of anti-HER2 affibody. Bioconjug Chem.
8 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
9 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
10 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
11 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
12 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.